# [^125^I]2-Iodo-N-[(S)-{(S)-1-methylpiperidin-2-yl}(phenyl)methyl]3-trifluoromethyl-benzamide

Chemical name: | [^125^I]2-Iodo-N-[(S)-{(S)-1-methylpiperidin-2-yl}(phenyl)methyl]3-trifluoromethyl-benzamide | [image]
Abbreviated name: | [^125^I]5 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Glycine transporter 1 (GlyT1) | [image]
Target Category: | Transporters | [image]
Method of detection: | Single-photon emission computed tomography (SPECT), planar imaging | [image]
Source of signal / contrast: | ^125^I | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of relevant compounds (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=glycine%20transporter%201%20and%20imaging)]

[^125^I]2-Iodo-N-[(S)-{(S)-1-methylpiperidin-2-yl}(phenyl)methyl]3-trifluoromethyl-benzamide, abbreviated as [^125^I]5, is a 2-iodo-substituted derivative of SSR504734, which was synthesized by Fuchigami et al. for imaging neuropsychiatric disorders by targeting glycine transporter 1 (GlyT1) (1).

Glycine is involved in excitatory and inhibitory neurotransmission in the mammalian central nervous system. Glycine metabolism is controlled by GlyT1 and glycine transporter 2 (GlyT2) (2). GlyT1 is widely distributed in the forebrain areas such as the cortex, hippocampus, and thalamus, as well as glycine-innervated regions such as the spinal cord, brainstem, and cerebellum (1, 3). This expression pattern of GlyT1, especially in the neocortex, is closely related to the distribution of glutamatergic N-methyl-D-aspartate receptors (NMDAR). NMDAR dysfunction has been shown to be involved in various disorders such as schizophrenia, stroke, Parkinson’s disease, and Alzheimer’s disease, while glycine modulates excitatory neurotransmission by acting as a necessary co-agonist for NMDAR in the frontal brain areas (4-6). In this process, GlyT1 is considered to play an important role by regulating glycine concentration (5, 7, 8).

Because of these findings, pharmacological manipulation of glycine-mediated neurotransmission with GlyT1 inhibitors has become an active field for the development of novel treatments for neuropsychiatric disorders, and evidence has demonstrated the beneficial effect of the inhibitors on the negative and cognitive symptoms of schizophrenia (3, 9). Meaningful progress has also been made in the development of imaging probes for GlyT1 to obtain the disease information and the occupancy of GlyT1 inhibitors in vivo (1, 10).

Depoortere et al. synthesized the piperidine benzamide derivative 2-chloro-N-[(S)-phenyl[(2S)-piperidin-2-yl] methyl]-3-trifluoromethyl benzamide (SSR504734) and determined that SSR504734 is a selective and reversible inhibitor of human, rat, and mouse GlyT1 (half-maximal inhibitory concentration (IC_50_) = 18, 15, and 38 nM, respectively) (9). SSR504734 reversibly blocks the cortical uptake of glycine, thus increasing the extracellular levels of glycine in prefrontal cortex, and it exhibits therapeutic activity in schizophrenia, anxiety, and depression models in rats (9). Recently, ^11^C-labeled SSR504734 and its derivatives have been shown to exhibit high brain uptake and accumulation in the monkey brain, consistent with the GlyT1 distribution (10). Fuchigami et al. labeled the SSR504734 derivatives for imaging purposes by introducing a radioiodine atom into their 2-position (1). These compounds, especially [^125^I]5, show high blood–brain barrier permeability and specific brain distribution in GlyT1-rich regions (1). This chapter summarizes the data obtained with [^125^I]5.

### Related Resource Links:

The protein (http://www.ncbi.nlm.nih.gov/protein/?term=glycine%20transporter%201) sequence of Gly T1

PubChem Bioassay data (http://www.ncbi.nlm.nih.gov/pcassay/?term=glycine%20transporter%201) of Gly T1

Gly T1 related clinical trials (http://clinicaltrials.gov/ct2/results?term=glycine+transporter) in ClinicalTrials.gov

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21975065)]

Fuchigami et al. described the synthesis of [^125^I]5 in detail (1). The compound (S)-{(S)-1-allylpiperidin-2-yl}(phenyl)methanamine was first prepared and then coupled with 3-trifluoromethyl-2-iodobenzoic acid (71% yield). Subsequent Pd(0)-catalyzed deprotection of the allyl group resulted in compound 3 (2-iodo-N-[(S)-{(S)-1-piperidin-2-yl}(phenyl)methyl]3-trifluoromethyl-benzamide; 88% yield). Reductive amination of SSR504734 and compound 3 yielded 94% of compound 4 (2-chloro-N-[(S)-{(S)-1-methylpiperidin-2-yl}(phenyl)methyl]3-trifluoromethyl-benzamide) and 95% of compound 5, respectively. Compound 4 is the N-methyl derivative, and compounds 3 and 5 are the 2-iodo-substituted derivatives of SSR504734.

The synthesis of [^125^I]5 from its tributyltin precursor was initially carried out; however, radioiodination of the tributyltin precursor did not proceed, probably due to steric hindrance of the precursor (data not shown). Therefore, Fuchigami et al. first prepared the trimethyltin precursor of compound 5via an iodo-to-trimethyltin exchange reaction (67% yield), and then generated the [^125^I]5 by reaction of the trimethyltin precursor and [^125^I]NaI (carrier-free) in the presence of chloramine-T and HCl at 60°C for 40 min (1). The radiochemical yield was 13%–19%, and the radiochemical purity was >98%. The lipophilicity (logD_7.4_) value of [^125^I]5 was 2.86 (detailed data not shown). The specific activity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21975065)]

Fuchigami et al. evaluated and compared the inhibitory activities on GlyT1 among five compounds (SSR504734, 3, 4, 5, and ALX5407) using a [^3^H]glycine uptake-JAR cell system (1). JAR is a human choriocarcinoma cell line that expresses GlyT1. ALX5407 is a first-generation GlyT1 inhibitor with high inhibitory potency, but its safety profile and pharmacokinetics in vivo are unfavorable (11). The inhibitory effect of each compound on [^3^H]glycine uptake was expressed as IC_50_ value (Table 1).

SSR504734 showed modest inhibitory activity, but its N-methyl derivative 4 showed 11-fold higher activity. Introduction of an iodine atom into the 2-position of SSR504734 resulted in the improvement of inhibitory activity (compounds 3 and 5). Compound 5 exhibited the best inhibitory activity, which was 18-fold and 3-fold higher than 3 and 4, respectively. These results indicate the importance of the methyl group for GlyT1 inhibition, and the iodine atom is preferred over the chloride atom for inhibitory activity. The inhibitory activity of ALX5407 was 6-fold higher than that of 5.

Table 1: Inhibition on [^3^H]glycine uptake of JAR cells.

Compound | SSR504734 | 3 | 4 | 5 | ALX5047
IC_50_ (nM) | 80.1 ± 7.55 | 43.0 ± 4.12 | 7.51 ± 1.91 | 2.35 ± 0.35 | 0.39 ± 0.05

The binding property of [^125^I]5 was investigated with rat cortical brain homogenates and saturation assay (1). The binding of [^125^I]5 was calculated to be a well-fitted one binding site model (R_2_ = 0.985) with high affinity (K_d_ = 1.58 ± 0.34 nM). The maximal binding value was estimated to be 3.40 ± 0.18 pmol/mg protein.

The in vitro brain distribution of [^125^I]5 was characterized with rat brain sections and autoradiography (1). The brain sections were incubated with [^125^I]5 (100 kBq (2.70 µCi)) (0.03–0.04 nM) for 30 min at 25°C. [^125^I]5 showed high accumulation in the corpus callosum, thalamus, midbrain, medullary, and cerebellar white matter, and low uptake in the cerebral cortex, hippocampus, striatum, and cerebellar gray matter. The accumulation pattern of [^125^I]5 was similar to the distribution of GlyT1 immunoreactivity in the rat brain. Nonspecific binding was determined in the presence of nonradioactive 5 (10 μM), which resulted in a significant reduction of radioactivity accumulation in the whole brain. Regional brain differences for [^125^I]5 binding disappeared. These results indicate that the binding of [^125^I]5 in the rat brain slices correlates with GlyT1 expression level.

The specificity of [^125^I]5 (100 kBq (2.70 µCi) (0.03–0.04 nM) binding to GlyT1 was examined with four GlyT1 inhibitors (SSR504734, compound 4, ALX5047, and HPCP ((+)-N-[cis-1-(2-hydroxy-2-phenyl-cyclohexyl)-piperidin-4-yl]-4-methoxy-N-phenyl-benzenesulfonamide), 10 μM/agent), one GlyT1 substrate (glycine, 1 mM or 10 mM), one GlyT2 inhibitor (ORG25543, 10 μM), and one NMDAR glycine site antagonist (L-701,324, 10 μM) (1). SSR504734 derivatives are competitive, and ALX5407 is a noncompetitive inhibitor of the GlyT1. HPCP has a different structure from [^125^I]5 (1).

SSR504734 and its N-methyl derivative 4 partially decreased the accumulation of [^125^I]5 in the GlyT1-rich regions, such as the corpus callosum, thalamus, midbrain, medullary, and cerebellum (21%−27% and 20%−29% compared with control, respectively; P < 0.05). Reduction of radioactivity was also observed in the GlyT1-poor regions, such as the cerebral cortex, hippocampus, and striatum (32%−45% and 32%−46% for SSR504734 and 4, respectively). HPCP showed partial inhibition of the [^125^I]5 binding to GlyT1-rich regions (11%−23%) and moderate inhibition to GlyT1-poor regions (31%−56%). ALX5407 decreased [^125^I]5 binding in all brain regions, though to a lower extent than other GlyT1 inhibitors, which is thought to be caused by allosteric inhibition of ALX5047 to the [^125^I]5 binding for GlyT1. Glycine had almost no effect on [^125^I]5 binding at 1 mM, and when increased to 10 mM glycine reduced the accumulated radioactivity in all brain regions. These results suggest that compound 5 is a competitive inhibitor of the glycine binding site of GlyT1 and that the binding affinity of glycine to the [^125^I]5 binding site is much lower than that of the GlyT1 inhibitors. ORG25543 and L-701,324 did not affect the [^125^I]5 binding in any brain regions.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21975065)]

The biodistribution of [^125^I]5 was studied in normal ddY mice (n = 5–6/time point) after tail vein injection of 11.1 kBq (0.3 µCi) [^125^I]5, and its accumulation in organs was expressed as percentage of injected dose per gram tissue (% ID/g) (1). High pulmonary uptake of [^125^I]5 was observed at all time points (9.34%−17.19% ID/g), which could be attributed to the piperidine moiety of this tracer. Initial brain uptake of [^125^I]5 was 0.51% ID/g (at 0.5 min), then increased over time and peaked at 2.42% ID/g at 30 min, suggesting good blood–brain barrier permeability of [^125^I]5. The brain uptake of [^125^I]5 gradually decreased after 30 min, but the brain–blood ratio remained constant for up to 60 min after injection (2.46 and 2.32 at 30 min and 60 min, respectively). High brain uptake of [^125^I]5 can be explained partially by its ideal lipophilicity. Radiotracers with moderate lipophilicity (logD_7.4_ values, 2.0–3.5) usually have optimal passive brain entry under in vivo condition.

Metabolism of [^125^I]5 in mouse brain was analyzed with brain homogenates obtained at different times after injection of [^125^I]5 (185 kBq (5 µCi)) and 92%, 90%, and 89% of [^125^I]5 remained unchanged at 5, 30, and 60 min after injection, respectively (data not shown), suggesting that metabolism should have little or no influence on the in vivo brain distribution pattern of [^125^I]5 (1).

The specificity of regional brain binding of [^125^I]5 (33.3 kBq (0.9 µCi)) for GlyT1 was analyzed with pre-administration of nonradioactive 5, compound 4, SSR504734, and ALX5407 (2 mg/kg per blocking agent), respectively, 15 min before injection of [^125^I]5 (n = 5–6 mice/time point per agent) (1). Because the brain/blood ratio of [^125^I]5 peaked at 30 min and 60 min in biodistribution studies, regional brain distribution studies were therefore conducted at 30 min and 60 min after the radiotracer injection. The blocking effect on [^125^I]5 accumulation was expressed as a percentage of the control (no administration of blocking agents) at 30 min and 60 min, respectively. The results showed that pre-injection of nonradioactive compound 5 resulted in partial reduction of [^125^I]5 accumulation in the GlyT1-rich regions, such as the thalamus (45% and 58%; P < 0.05), midbrain (48% and 51%; P < 0.05), and medulla (53% and 52%; P < 0.05). In contrast, the extent of [^125^I]5 uptake reduction in the GlyT1-poor regions, such as the hippocampus and striatum, was relatively lower than the GlyT1-rich regions. Pre-administration of compound 4 also led to a partial decrease in regional radioactivity uptake in the thalamus (56% and 56%; P < 0.05), midbrain (55% and 48%; P < 0.05), and medulla (59% and 47%; P < 0.05), but also resulted in little displacement of radioactivity from the hippocampus and striatum. The estimated brain region/blood ratios were also significantly decreased by nonradioactive compound 5 and compound 4 in the GlyT1-rich regions. The radioactivity level of [^125^I]5 in all brain regions became homogenous with the use of these blockers. These results indicate that in vivo binding of [^125^I]5 is specifically mediated by GlyT1. SSR504734 did not significantly block the uptake of [^125^I]5 in any brain regions (P > 0.05), which might be due to its much lower inhibitory activity and binding affinity for GlyT1 than its N-methyl analogs (compounds 4 and 5). Pretreatment with ALX5407 showed no effect on the brain uptake of [^125^I]5 at 30 min and weak inhibitory effect at 60 min (P > 0.05).

Fuchigami et al. further investigated the in vivo binding properties of [^125^I]5 to GlyT1 with ex vivo autoradiography (1). Mice (n = 5) were injected intravenously with [^125^I]5 (200 kBq (5.41 µCi)) and euthanized at 60 min after administration. The results showed high uptake of [^125^I]5 in the GlyT1-rich regions (thalamus, midbrain, cerebellum, and medullary) and low uptake in the GlyT1-poor regions (cerebral cortex, hippocampus, and striatum). The low radioactivity of [^125^I]5 in the corpus callosum was inconsistent with that obtained in the in vitro autoradiography studies, which might be due to the influence of lower regional blood flow in the white matter, such as the corpus callosum, than in other brain regions. To further confirm the in vivo specificity of [^125^I]5 for GlyT1, blocking studies were performed by pretreatment with nonradioactive compound 5 or compound 4 (2 mg/kg body weight) 15 min before [^125^I]5 injection (n = 5 mice/group). Both compound 5 and compound 4 abolished the heterogenous distribution of [^125^I]5 in the brain regions. Accumulation of [^125^I]5 was significantly reduced by these compounds only in the GlyT1-rich regions (P < 0.05).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

No references are currently available.

## References

1 Fuchigami T., Haratake M., Magata Y., Haradahira T., Nakayama M. (2011). Synthesis and characterization of [(1)(2)I]2-iodo N-[(S)-{(S)-1-methylpiperidin-2-yl}(phenyl)methyl]3-trifluoromethyl-benzamide as novel imaging probe for glycine transporter 1. Bioorg Med Chem.
2 Zafra F., Gimenez C. (2008). Glycine transporters and synaptic function. IUBMB Life.
3 Wolkenberg S.E., Sur C. (2010). Recent progress in the discovery of non-sarcosine based GlyT1 inhibitors. Curr Top Med Chem.
4 Sur C., Kinney G.G. (2007). Glycine transporter 1 inhibitors and modulation of NMDA receptor-mediated excitatory neurotransmission. Curr Drug Targets.
5 Gomeza, J.,Armsen, W.,Betz, H., and Eulenburg, V. Lessons from the knocked-out glycine transporters. Handb Exp Pharmacol. 2006(175): 457-83.
6 Eulenburg V., Gomeza J. (2010). Neurotransmitter transporters expressed in glial cells as regulators of synapse function. Brain Res Rev.
7 Betz H., Laube B. (2006). Glycine receptors: recent insights into their structural organization and functional diversity. J Neurochem.
8 Betz H., Gomeza J., Armsen W., Scholze P., Eulenburg V. (2006). Glycine transporters: essential regulators of synaptic transmission. Biochem Soc Trans.
9 Depoortere R., Dargazanli G., Estenne-Bouhtou G., Coste A., Lanneau C., Desvignes C., Poncelet M., Heaulme M., Santucci V., Decobert M., Cudennec A., Voltz C., Boulay D., Terranova J.P., Stemmelin J., Roger P., Marabout B., Sevrin M., Vige X., Biton B., Steinberg R., Francon D., Alonso R., Avenet P., Oury-Donat F., Perrault G., Griebel G., George P., Soubrie P., Scatton B. (2005). Neurochemical, electrophysiological and pharmacological profiles of the selective inhibitor of the glycine transporter-1 SSR504734, a potential new type of antipsychotic. Neuropsychopharmacology.
10 Toyohara J., Ishiwata K., Sakata M., Wu J., Nishiyama S., Tsukada H., Hashimoto K. (2011). In vivo evaluation of carbon-11-labelled non-sarcosine-based glycine transporter 1 inhibitors in mice and conscious monkeys. Nucl Med Biol.
11 Perry K.W., Falcone J.F., Fell M.J., Ryder J.W., Yu H., Love P.L., Katner J., Gordon K.D., Wade M.R., Man T., Nomikos G.G., Phebus L.A., Cauvin A.J., Johnson K.W., Jones C.K., Hoffmann B.J., Sandusky G.E., Walter M.W., Porter W.J., Yang L., Merchant K.M., Shannon H.E., Svensson K.A. (2008). Neurochemical and behavioral profiling of the selective GlyT1 inhibitors ALX5407 and LY2365109 indicate a preferential action in caudal vs. cortical brain areas. Neuropharmacology.